# ^99m^Tc-Anti-ED-B fibronectin L19-(Gy)_3_-Cys-Ala scFv antibody fragment

Chemical name: | ^99m^Tc-Anti-ED-B fibronectin L19-(Gy)_3_-Cys-Ala scFv antibody fragment
Abbreviated name: | ^99m^Tc-AP39
Synonym: | ^99m^Tc-scFv L19, ^99m^Tc-anti-ED-B FN scFv Ab
Agent Category: | Single-chain Antibody fragment (scFv)
Target: | ED-B Fibronectin (FN)
Target Category: | Antibody-antigen binding
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=5725426), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=31406) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=407105) for more information about ED-B fibronectin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2899mTc-AP39%29%20OR%20%28Radiolabeled%20anti-fibronectin%20antibody%29)]

^99m^Tc-Anti-ED-B fibronectin L19-(Gly)_3_-Cys-Ala scFv antibody fragment (^99m^Tc-AP39) is a radiolabeled molecular imaging agent developed for single-photon emission computed tomography (SPECT) imaging of tumor angiogenesis and guidance in antiangiogenic treatment (1). ^99m^Tc is a gamma emitter with a half-life (t_½_) of 6.02 h.

Angiogenesis is a process of development and growth of new blood vessels from pre-existing vessels (2). Tumor growth depends on the formation of new blood vessels via this process. Normal angiogenesis is orderly and highly regulated, whereas tumor angiogenesis is chaotic and irregular. Abnormal angiogenesis is important in the carcinogenesis, growth and progression of human solid and hematologic tumors (3). Fibronectins (FNs) are a widely distributed family of universal cell-adhesion molecules (1). FN is a polymorphic glycoprotein of ~2500 amino acids and has a high molecular mass of 250−280 kDa. FN occurs in soluble form in plasma and other body fluids and in insoluble form in the extracellular matrixes (4, 5). Both forms are dimers composed of a series of repeating units of three types and joined by two disulfide bonds at the carboxyl terminus of the molecule. FN polymorphism arises from alternative splicing patterns of the pre-mRNA or post-translational modifications of FN itself (5). Alternative splicing in three different regions may generate 20 different FN subunit isoforms. The splice variant ED-B FN, which is highly expressed during angiogenesis in both neoplastic and normal tissues (6), is an oncofetal antigen expressed at different levels in the stroma associated with the neovasculature of solid tumors. High levels of ED-B expression have been found in primary and metastatic tumors in breast, colorectal, and non-small cell lung cancer (1, 7-9).

Molecular imaging of angiogenesis offers serial non-invasive evaluation of both location and growth dynamics of tumors (10) SPECT or positron emission tomography imaging with the appropriate radiolabeled tracer targeted to angiogenic pathways may allow the evaluation of specific aspects of tumor vascular biology (9). A molecular probe that targets ED-B FN can be both an early tumor marker and a tool to monitor the success of antiangiogenic cancer therapy. The single-chain antibody fragment (scFv), L19, with a high affinity to ED-B FN was developed by Pini et al. (11). Radioiodinated L19 showed specific accumulation around tumor neovasculature and tumor stroma with high ED-B expression (12, 13). In an effort to prepare a stable ^99m^Tc-labeled L19, Berndorff et al. (1) inserted the amino acid sequence (Gly)3-Cys-Ala at the C terminus of L19 to produce the recombinant protein, AP39 The authors suggested that a ^99m^Tc(V) oxo metal complex could be formed. ^99m^Tc-AP39 appeared to have favorable biodistribution and imaging properties in mice bearing murine embryonal teratocarcinoma (F9).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2899mTc-AP39%29%20OR%20%28Radiolabeled%20anti-fibronectin%20antibody%29%29%20AND%20synthesis)]

Pini et al. (11) constructed and used a large synthetic phage display human antibody library (>3 x 10^8^ clones) to produce L19 with a very high affinity of dissociation constant (K_d_) of 54 pM to the ED-B domain of FN. L19 was cloned in scFv configuration in the novel phagemid vector, pDN332. Berndorff et al. (1) prepared the L19 derivative by modifying the sequence of scFv LP19 to encode the ^99m^Tc binding motif (Gly)_3_-Cys-Ala at the C-terminal end of the VL chain. The DNA sequence encoding this LP19 derivative was cloned into the prokaryotic expression vector pDN5 with isopropyl-1-thio-β-D-galactoside (IPTG)-inducible promoter and the ampicillin resistance marker.AP39 was isolated and purified from the soluble fraction of the French press lysate of the Escherichia coli culture. Before radiolabeling, AP39 was reduced by Tris-(2-carboxyethyl)phosphine hydrochloride (TCEP) in sodium phosphate (Na_2_HPO_4_) buffer (pH 7.4). The reaction mixture was gently shaken for 1 h at room temperature. TCEP was then removed by chromatography. Sodium dodecyl sulfate/polyacrylamide gel electrophoresis of the purified product confirmed the transformation of the S-S-dimeric AP39 to the SH-monomeric AP39 and associative dimer form. For radiolabeling, reduced AP39 in phosphate- buffered saline was added to disodium-L-tartrate and diluted with Na_2_HPO_4_ buffer. ^99m^Tc pertechnetate and tin-II chloride (SnCl_2_ in 0.1 mol/L hydrochloric acid) were added. The reaction mixture was shaken for 30 min at 37ºC. ^99m^Tc-AP39 was purified by gel chromatography. The radiochemical yield was >50% after purification. The radiochemical purity was >95%. By high-performance liquid chromatography analysis, ^99m^Tc-AP39 appeared to be a mixture of predominantly dimeric (~80%) and monomeric (~16%) ^99m^Tc-AP39. The specific activity of ^99m^Tc-AP39 was 35 MBq/nmol [0.95 mCi/nmol(dimer)].

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2899mTc-AP39%29%20OR%20%28Radiolabeled%20anti-fibronectin%20antibody%29%29%20AND%20in%20vitro)]

Berndorff et al. (1) determined the in vitro immunoreactivity of ^99m^Tc-AP39 by using affinity chromatography with ED-B FN-conjugated Sepharose. ^99m^Tc-AP39 showed an immunoreactivity of 96%.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2899mTc-AP39%29%20OR%20%28Radiolabeled%20anti-fibronectin%20antibody%29%29%20AND%20rodentia)]

Biodistribution studies (n = 3) of ^99m^Tc-AP39 were performed in nude mice bearing the murine teratocarcinoma F9 (1). F9 tumors were previously reported to express high levels of ED-B FN (13). ^99m^Tc-AP39 showed rapid blood clearance and radioactivity localization in the tumor. The radioactivity levels of ^99m^Tc-AP39 in percentage of the injected dose per g (% ID/g) in the tumor were 5.2 ± 2.5 (0.25 h), 6.1 ± 2.0 (1 h), 8.3 ± 3.2 (3 h), 8.7 ± 52.5 (5 h), and 2.8 ± 1.4 (24 h). The tumor/blood ratios were 0.4 ± 0.2 (0.25 h), 1.6 ± 0.2 (1 h), 6.4 ± 2.9 (3 h), 9.0 ± 6.5 (5 h), and 17.2 ± 6.8 (24 h). ^99m^Tc-AP39 appeared to be excreted primarily by the kidneys. The radioactivity levels (% ID/g) in the kidneys were 48.2 ± 4.2 (0.25 h), 21.8 ± 2.5 (1 h), 8.6 ± 0.6 (3 h), 7.9 ± 0.4 (5 h), and 2.6 ± 0.4 (24 h). About 64.5% ID was excreted via the urine after 24 h. There was little radioactivity accumulation in other nontarget organs. The authors suggested that the absence of radioactivity in the thyroid indicated no significant release of unlabeled ^99m^Tc from ^99m^Tc-AP39.

Gamma imaging was performed in mice bearing 80−100 mm^2^ s.c.F9 tumors (1). Each mouse was injected with 4−7 MBq (0.11−0.19 mCi) ^99m^Tc-AP39. Imaging with ^99m^Tc-AP39 gave clear tumor images for at least 24 h with low background radioactivities. The kidneys were visualized at 3 and 5 h. The liver and bladder were the only other organs weakly detected at early time points.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2899mTc-AP39%29%20OR%20%28Radiolabeled%20anti-fibronectin%20antibody%29%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2899mTc-AP39%29%20OR%20%28Radiolabeled%20anti-fibronectin%20antibody%29%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2899mTc-AP39%29%20OR%20%28Radiolabeled%20anti-fibronectin%20antibody%29%29%20AND%20human)]

No publication is currently available.

## References

1 Berndorff D., Borkowski S., Moosmayer D., Viti F., Muller-Tiemann B., Sieger S., Friebe M., Hilger C.S., Zardi L., Neri D., Dinkelborg L.M. (2006). Imaging of tumor angiogenesis using 99mTc-labeled human recombinant anti-ED-B fibronectin antibody fragments. J Nucl Med.
2 Shinkaruk S., Bayle M., Lain G., Deleris G. (2003). Vascular endothelial cell growth factor (VEGF), an emerging target for cancer chemotherapy. Curr Med Chem Anticancer Agents.
3 Ranieri G., Patruno R., Ruggieri E., Montemurro S., Valerio P., Ribatti D. (2006). Vascular endothelial growth factor (VEGF) as a target of bevacizumab in cancer: from the biology to the clinic. Curr Med Chem.
4 Carnemolla B., Balza E., Siri A., Zardi L., Nicotra M.R., Bigotti A., Natali P.G. (1989). A tumor-associated fibronectin isoform generated by alternative splicing of messenger RNA precursors. J Cell Biol.
5 Kosmehl H., Berndt A., Katenkamp D. (1996). Molecular variants of fibronectin and laminin: structure, physiological occurrence and histopathological aspects. Virchows Arch.
6 Castellani P., Viale G., Dorcaratto A., Nicolo G., Kaczmarek J., Querze G., Zardi L. (1994). The fibronectin isoform containing the ED-B oncofetal domain: a marker of angiogenesis. Int J Cancer.
7 Kaczmarek J., Castellani P., Nicolo G., Spina B., Allemanni G., Zardi L. (1994). Distribution of oncofetal fibronectin isoforms in normal, hyperplastic and neoplastic human breast tissues. Int J Cancer.
8 Pujuguet P., Hammann A., Moutet M., Samuel J.L., Martin F., Martin M. (1996). Expression of fibronectin ED-A+ and ED-B+ isoforms by human and experimental colorectal cancer. Contribution of cancer cells and tumor-associated myofibroblasts. Am J Pathol.
9 Santimaria M., Moscatelli G., Viale G.L., Giovannoni L., Neri G., Viti F., Leprini A., Borsi L., Castellani P., Zardi L., Neri D., Riva P. (2003). Immunoscintigraphic detection of the ED-B domain of fibronectin, a marker of angiogenesis, in patients with cancer. Clin Cancer Res.
10. Laking, G.R. and P.M. Price, Positron emission tomographic imaging of angiogenesis and vascular function. Br J Radiol, 2003. 76 Spec No 1: p. S50-9.
11 Pini A., Viti F., Santucci A., Carnemolla B., Zardi L., Neri P., Neri D. (1998). Design and use of a phage display library. Human antibodies with subnanomolar affinity against a marker of angiogenesis eluted from a two-dimensional gel. J Biol Chem.
12 Tarli L., Balza E., Viti F., Borsi L., Castellani P., Berndorff D., Dinkelborg L., Neri D., Zardi L. (1999). A high-affinity human antibody that targets tumoral blood vessels. Blood.
13 Borsi L., Balza E., Bestagno M., Castellani P., Carnemolla B., Biro A., Leprini A., Sepulveda J., Burrone O., Neri D., Zardi L. (2002). Selective targeting of tumoral vasculature: comparison of different formats of an antibody (L19) to the ED-B domain of fibronectin. Int J Cancer.